# 2-{3-[^18^F]Fluoro-4-(methylamino)phenyl}-1,3-benzothiazol-6-ol

Chemical name: | 2-{3-[^18^F]Fluoro-4-(methylamino)phenyl}-1,3-benzothiazol-6-ol | [image]
Abbreviated name: | [^18^F]Flutemetamol | [image]
Synonym: | [^18^F]AH110690; [^18^F]-3'-F-6-OH-BTA1; [^18^F]-GE067 | [image]
Agent Category: | Compound | [image]
Target: | β-Amyloid plaque | [image]
Target Category: | Protein | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - Rodents; - Humans | Structure of [^18^F]flutemetamol.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=flutemetamol%20pet&cmd=DetailsSearch)]

Development of Alzheimer's disease (AD) has been attributed to neurodegeneration as a result of the neuronal overexpression, secretion, and deposition of the neurotoxic amyloid β (Aβ) fragment of the Aβ protein precursor in the brain (1). No specific treatment for AD is currently available, and clinicians are increasingly focused on developing ways to either prevent or delay the formation of Aβ plaques in the brain of AD patients (2). In addition, several hundred clinical trials (http://clinicaltrials.gov/ct2/results?term=Alzheimer%E2%80%99s+disease+) approved by the United States Food and Drug Administration have been completed or are in progress to develop drugs for the prevention, onset delay, or treatment of AD. Early detection of Aβ plaques by noninvasive techniques such as positron emission tomography (PET) are often used to identify individuals who are prone to develop the disease and to monitor the efficacy of drugs used to treat or delay onset of the disease (3).

The ^11^C-labeled Pittsburgh compound B ([^11^C]PIB (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PIB11C)) is the most commonly used PET tracer for the detection of Aβ plaques, but the short half-life of ^11^C (20.4 min) restricts the use of this label to clinical facilities that have the capability to generate the probe on site (3). Some ^18^F-labeled compounds (half-life of ^18^F is ~110 min) have also been generated for the visualization of Aβ plaques, but these labeled compounds usually show low specificity toward the plaques (3). Investigators have synthesized some ^18^F-labeled PIB analogs, such as [^18^F]BAY94-9172 (4) and [^18^F]flutemetamol (2-{3-[^18^F]Fluoro-4-(methylamino)phenyl}-1,3-benzothiazol-6-ol) (5), earlier known as [^18^F]GE067 (6), and are evaluating these probes for the detection and diagnosis of AD in the clinic. Flutemetamol is a thioflavin T derivative of PIB and bears ^18^F-fluorine on the 3' position of the parent molecule (7). The biodistribution and PET imaging of Aβ plaques with [^18^F]flutemetamol have been investigated in rodents (8), healthy human volunteers (5, 6), and patients with mild cognitive impairment (7) and AD (5, 6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

What is Alzheimer's disease (AD) (http://www.nlm.nih.gov/medlineplus/alzheimersdisease.html)?; Alzheimer's disease in Genetics Home Reference (http://ghr.nlm.nih.gov/condition/alzheimer-disease); Alzheimer's disease in Genome Wide Association Studies (http://www.genome.gov/gwastudies/index.cfm?#searchForm) database

β-Amyloid (A4) precursor protein gene information (http://www.ncbi.nlm.nih.gov/gene/351) (Gene ID 351)

Information on amyloidosis and related topics in Online Mendelian Inheritance in Man (OMIM) Database (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=Amyloid) related to β-amyloid plaques

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Flutemetamol&Search=Search) related to [^18^F]flutemetamol

Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16) on U.S. Food and Drug Administration web site

Partial structure of β-amyloid protein (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=92080) (Protein Data Bank, NCBI)

FDA-approved treatments (http://www.alz.org/national/documents/topicsheet_treatments.pdf) for Alzheimer's disease (from Alzheimer's Association web site; www.alz.org)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20synthesis&cmd=DetailsSearch)]

Snellman et al. (8) synthesized [^18^F]flutemetamol according to a procedure similar to that described in patent WO 2007/020400 A1 (9). The specific activity (SA) of [^18^F]flutemetamol was reported to be 1,460 ± 1,160 GBq/μmol (54.02 ± 42.92 Ci/μmol) at the end of synthesis (EOS) and 980 ± 430 GBq/μmol (36.26 ± 15.91 Ci/μmol) at the time of injection. The radiochemical purity (RCP) of the purified product was >98%. The radiochemical yield (RCY) and stability of the tracer were not reported.

[^11^C]PIB was synthesized and used for comparison with [^18^F]flutemetamol in some studies (8). The SA of [^11^C]PIB was reported to be 50 ± 11 GBq/μmol (1.85 ± 0.41 Ci/μmol) at the EOS and 17 ± 5 GBq/μmol (0.63 ± 0.19 Ci/μmol) at the time of injection. The RCP of [^11^C]PIB was >95%, but the RCY and stability of the tracer were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20in%20vitro%20studies&cmd=DetailsSearch)]

No reference is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]flutemetamol was compared with that of [^11^C]PIB in Sprague-Dawley rats (8). The animals (n = 3–5 rats/time point for each tracer) were administered 36 ± 7 MBq (1.33 ± 0.26 mCi; 0.05 ± 0.02 ng/g body weight (BW)) [^18^F]flutemetamol or 32 ± 8 MBq (1.18 ± 0.3 mCi; 2.7 ± 1.2 ng/g BW) [^11^C]PIB through the tail vein, and the mice were euthanized at various time points ranging from 5 min postinjection (p.i.) to 60 min p.i. (for [^11^C]PIB) or 120 min p.i. (for [^18^F]flutemetamol). All organs of interest, including the brain, were harvested from the rodents to determine the uptake of radioactivity in the various tissues. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). Radioactivity from both [^18^F]flutemetamol and [^11^C]PIB was rapidly cleared from blood and the other peripheral organs. Maximum tracer accumulation at 5 min p.i. was detected in the liver, and later in the intestine and the kidney from 30 min p.i. to 60 min p.i. Very little ^18^F was detected in the bones, indicating that [^18^F]flutemetamol was not defluorinated while in circulation. With [^18^F]flutemetamol, the uptake of label in the brain peaked at 5 min p.i. (3.67 ± 1.69% ID/g), and the brain/blood (BB) ratio at this time point was 12.2, which decreased to 4.6 at 15 min p.i. and to 1.0 at 60 min p.i. The frontal cortex of the brain showed the highest accumulation of label (at 5 min p.i.), followed by the striatum (from 15 min p.i. to 60 min p.i.). The uptake of tracer with [^11^C]PIB peaked at 5 min p.i. in the brain, with a BB ratio of 4.4, which decreased to 2.4 at 15 min p.i. and to 1.1 at 60 min p.i.

Autoradiographic images of brain sections obtained from the animals showed that the clearance of [^18^F]flutemetamol, particularly from the white matter, was slower than that of [^11^C]PIB (8). From the images it was evident that the uptake of label from [^11^C]PIB was homogeneous in all areas of the brain, but with [^18^F]flutemetamol the accumulation of radioactivity was higher in the white matter than in the gray matter. With [^18^F]flutemetamol, the white matter/parietal cortex ratio increased from 0.6 at 5 min p.i. to 1.6 at 30 min p.i. and to 10.9 at 60 min p.i. For [^11^C]PIB, this ratio increased from 1.1 at 5 min p.i. to 3.7 at 30 min p.i. (the ratio at 60 min p.i. was not reported because there was very low uptake of label in the brain at this time point).

To confirm that [^18^F]flutemetamol and [^11^C]PIB targeted the Aβ deposits in the brains of transgenic mice that are prone to develop AD (Tg2576 mice (http://www.criver.com/en-US/ProdServ/ByType/Discovery/CNS/Alzheimers/Pages/Tg2576_Mouse.aspx)), the animals were injected with the radiochemicals as before (8). The brains of the animals were removed, and brain sections were subject to ex vivo autoradiography as described elsewhere (8). The radiographic images showed that both tracers were bound to the Aβ deposits present in the pre-frontal cortex of the animals. Preincubation of the brain sections with nonradioactive PIB resulted in displacement of radioactivity from the Aβ plaques. This showed that both radiochemicals had a high binding specificity for the Aβ deposits in the brain. The location of the plaques visualized with the two tracers was confirmed by staining the same brain sections with thioflavin S and the 6E10 monoclonal antibody (https://store.crpinc.com/datasheet.aspx?catalogno=sig-39320). Autoradiography of the sections revealed that the nonspecific binding of [^18^F]flutemetamol in the white matter of the brain was higher than that observed with [^11^C]PIB in the same regions.

From these studies, the investigators concluded that [^18^F]flutemetamol is probably suitable for the visualization of Aβ plaques in the brains of rodents (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b18F%5dflutemetamol%20Human%20Studies&cmd=DetailsSearch)]

In a phase I clinical study, the biodistribution of [^18^F]flutemetamol was investigated in 6 healthy elderly human subjects (5 men and 1 woman; age range, 51–74 yrs) by Koole et al. (6). On average, the subjects received 121 MBq (~4.5 mCi) [^18^F]flutemetamol in the presence of 10 μg nonradioactive flutemetamol as a slow bolus injection through the antecubital vein. Whole-body PET scans were obtained from the individuals as described by van Laere et al. (10). From the images it was evident that the label was taken up by the brain (6%–8% ID/g) and the liver (~25% ID/g) at <5 min p.i., and the tracer was gradually lost from both of these organs by 5 h p.i. At 60 min p.i., the amount of radioactivity accumulated in the gall bladder was <1% ID/g for 2 patients and 5%–13% ID/g in the other 4 patients). The amount of label in the intestine at 60 min p.i. varied from ~2% ID/g (2 patients) to 20%–40% ID/g (4 patients), and in the urinary bladder the uptake was ~5% ID/g in all patients at this time point. For most patients, the accumulation of radioactivity gradually increased in the gall bladder, intestine, and the urinary bladder from 60 min p.i. to 5 h p.i. From this study, the investigators concluded that [^18^F]flutemetamol was safe to use in humans and was probably suitable for the imaging of Aβ plaques in the human brain (6).

In another phase I clinical study, the use of [^18^F]flutemetamol for the detection of AD in humans was investigated in 8 patients with clinical early-stage probable AD (6 men and 2 women; mean age, 68.8 yrs) and 8 healthy controls (5 men and 3 women; mean age, 62.5 yrs) (5). All participants in the study received a slow bolus injection of ~180 MBq (6.66 mCi) [^18^F]flutemetamol through the antecubital vein, and brain PET scans were acquired from the individuals as described elsewhere (5). It was observed that, after 80 min p.i., the neocortical to cerebral uptake was maximal in both groups and was not affected by the start time or duration of the scan. However, the AD patients showed significantly higher standardized uptake value ratios (SUVRs) in the neocortical association zones and the striatum compared with the controls. There was no difference in the uptake of radioactivity in the white matter, cerebellum, and pons of the brain between the two groups. Two patients with AD were false-negative with [^18^F]flutemetamol, and one control patient was false-positive with the tracer. From this study, the investigators concluded that the binding of [^18^F]flutemetamol in the human brain can be quantified, but further studies are necessary to validate its use as a biomarker for Aβ amyloidosis (5).

The efficacy of [^18^F]flutemetamol was compared with that of [^11^C]PIB for the imaging of AD and amnestic mild cognitive impairment (MCI) in a multicenter phase II clinical trial involving 27 patients with early-stage clinically probable AD, 20 individuals with MCI, and 15 healthy volunteers (7). The SUVRs for the AD and MCI subjects were determined and compared, and the test-retest variability of [^18^F]flutemetamol was determined in 5 of the AD patients. Results obtained from this study showed that SUVRs for the two probes were similar within the same subjects, and the Pearson correlation coefficients for the cortical region, lateral frontal region, striatum, and the subcortical white matter were 0.905, 0.924, 0.843, and 0.364, respectively. The test-retest variability of [^18^F]flutemetamol for the 5 AD patients ranged from 1% to 5%, indicating that there was a high test-retest reliability with this radiochemical. From this study, the investigators concluded that [^18^F]flutemetamol is probably well suited for the detection and diagnosis of AD in humans (7).

The correlation between PET imaging of Aβ plaques with [^18^F]flutemetamol and in vivo cerebral cortical histopathology was investigated in 7 patients with AD who had previously undergone biopsy for diagnosis of the disease (11). Each subject received a dose of ~185 MBq (6.84 mCi) [^18^F]flutemetamol, and whole-brain PET scans were obtained at ~90 min p.i. The investigators reported that there was a significant agreement (P = 0.01) between visual reads of the PET scans and the brain histopathology data of the patients. This indicated that [^18^F]flutemetamol has a high sensitivity for the detection of amyloid plaques.

In another [^18^F]flutemetamol PET imaging study with 12 patients of AD with normal pressure hydrocephalus, the brain uptake SUVRs correlated significantly (P = 0.0174) with the level of amyloid plaques observed with immunohistochemical staining (using the anti-amyloid 4 G8 monoclonal antibody (http://www.cellsciences.com/content/p-detail.asp?rowid=8056)) of brain biopsy samples of the patients (12).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bissette G. (2009). Does Alzheimer's disease result from attempts at repair or protection after transient stress?. J Alzheimers Dis.
2 Sano M., Grossman H., Van Dyk K. (2008). Preventing Alzheimer's disease : separating fact from fiction. CNS Drugs.
3 Serdons K., Van Laere K., Janssen P., Kung H.F., Bormans G., Verbruggen A. (2009). Synthesis and evaluation of three 18F-labeled aminophenylbenzothiazoles as amyloid imaging agents. J Med Chem.
4 Rowe C.C., Ackerman U., Browne W., Mulligan R., Pike K.L., O'Keefe G., Tochon-Danguy H., Chan G., Berlangieri S.U., Jones G., Dickinson-Rowe K.L., Kung H.P., Zhang W., Kung M.P., Skovronsky D., Dyrks T., Holl G., Krause S., Friebe M., Lehman L., Lindemann S., Dinkelborg L.M., Masters C.L., Villemagne V.L. (2008). Imaging of amyloid beta in Alzheimer's disease with 18F-BAY94-9172, a novel PET tracer: proof of mechanism. Lancet Neurol.
5 Nelissen N., Van Laere K., Thurfjell L., Owenius R., Vandenbulcke M., Koole M., Bormans G., Brooks D.J., Vandenberghe R. (2009). Phase 1 study of the Pittsburgh compound B derivative 18F-flutemetamol in healthy volunteers and patients with probable Alzheimer disease. J Nucl Med.
6 Koole M., Lewis D.M., Buckley C., Nelissen N., Vandenbulcke M., Brooks D.J., Vandenberghe R., Van Laere K. (2009). Whole-body biodistribution and radiation dosimetry of 18F-GE067: a radioligand for in vivo brain amyloid imaging. J Nucl Med.
7 Vandenberghe R., Van Laere K., Ivanoiu A., Salmon E., Bastin C., Triau E., Hasselbalch S., Law I., Andersen A., Korner A., Minthon L., Garraux G., Nelissen N., Bormans G., Buckley C., Owenius R., Thurfjell L., Farrar G., Brooks D.J. (2010). 18F-flutemetamol amyloid imaging in Alzheimer disease and mild cognitive impairment: a phase 2 trial. Ann Neurol.
8 Snellman A., Rokka J., Lopez-Picon F.R., Eskola O., Wilson I., Farrar G., Scheinin M., Solin O., Rinne J.O., Haaparanta-Solin M. (2012). Pharmacokinetics of [(18)F]flutemetamol in wild-type rodents and its binding to beta amyloid deposits in a mouse model of Alzheimer's disease. Eur J Nucl Med Mol Imaging.
9 . Storey, A.E., C.L. Jones, D.R.C. Bouvet, N. Lasbistes, S.M. Fairway, L. Williams, A.M. Gibson, R.J. Nairen, and F. KarimiI, Fluorination process of anilide derivatives and benzothiazole fluorinate derivatives as in vivo imaging agents., in World Intellectual Property Organization, W.I.P. Organization, Editor. 2007, General Electric: Great Britain.
10 Van Laere K., Koole M., Sanabria Bohorquez S.M., Goffin K., Guenther I., Belanger M.J., Cote J., Rothenberg P., De Lepeleire I., Grachev I.D., Hargreaves R.J., Bormans G., Burns H.D. (2008). Whole-body biodistribution and radiation dosimetry of the human cannabinoid type-1 receptor ligand 18F-MK-9470 in healthy subjects. J Nucl Med.
11 Wolk D.A., Grachev I.D., Buckley C., Kazi H., Grady M.S., Trojanowski J.Q., Hamilton R.H., Sherwin P., McLain R., Arnold S.E. (2011). Association between in vivo fluorine 18-labeled flutemetamol amyloid positron emission tomography imaging and in vivo cerebral cortical histopathology. Arch Neurol.
12 Wong, D.F., A.R. Moghekar, D. Rigamonti, J.R. Brasic, O. Rousset, W. Willis, C. Buckley, A. Smith, B. Gok, P. Sherwin, and I.D. Grachev, An In Vivo Evaluation of Cerebral Cortical Amyloid with [(18)F]Flutemetamol Using Positron Emission Tomography Compared with Parietal Biopsy Samples in Living Normal Pressure Hydrocephalus Patients. Mol Imaging Biol, 2012